# [^11^C]4-N-Methylamino-4´-hydroxystilbene

Chemical name: | [^11^C]4-N-Methylamino-4´-hydroxystilbene
Abbreviated name: | [^11^C]SB-13
Synonym:
Agent Category: | Compound
Target: | Aggregates of β-amyloid (Aβ) peptides
Target Category: | Acceptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20OR%20SB-13)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1, 2). It is characterized by the presence, in the brain, of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments containing the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation and Aβ deposits (7). The first successful agent used in human studies was [^18^F]FDDNP (8), a malonitrile derivative found to bind to both neurofibrillary tangles and β-amyloid plaques. The second successful attempt was made with [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1. [^11^C]PIB showed marked retention in areas of association cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13.

SB-13 can be labeled with either I-123 or C-11 for in vivo imaging using photon emission computerized tomography or PET. Research studies reported in the literature showed that [^11^C]SB-13 has selective high-affinity binding to amyloid plaques and demonstrated in vivo properties similar to those of [^11^C]PIB when used in AD patients.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

[^11^C]SB-13 can be synthesized from 4-amino-4´-hydroxystilbene and [^11^C]methyl triflate, as described by Ono et al. (10). The synthetic procedure uses the ”LOOP” method by which trapping and reaction of the [^11^C]-methylating agent and precursor are performed inside a high-performance liquid chromatography loop (11). In their experiments, the authors were able to obtain the final product, [^11^C]SB-13, with a radiochemical yield ranging from 13 to 15% (uncorrected, from [^11^C]CO_2_) and a total synthesis time of 23 min. The radiochemical purity obtained was >98%, and the specific activity at the end of the procedure ranged from 40 to 60 GBq/mmol (1,081 to 1,621 mCi/μmol).

A measure of the partition coefficient (P) for [^11^C]SB-13 (between 1-octanol and phosphate buffer at pH 7.4), following the described method (12), led to a moderate log(P) of 2.36 ± 0.04, suitable for brain imaging.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20in%20vitro)]

In vitro binding assays using preformed Aβ aggregates showed that [^11^C]SB-13 had very good binding affinities for amyloid plaques while competing with the radioiodinated benzothiazole [^125^I]2-(4´-dimethylaminophenyl)-6-iodobenzothiazole ([^125^I]TZDM). Its inhibition coefficient (K_i_) was found to be 6.0 ± 1.5 nM (at 25 °C) (10). In another experiment using brain sections of double-mutation mice (TgCRDN8) containing thioflavin S-positive Aβ plaques (10), [^11^C]SB-13 showed excellent binding properties in the mutant mouse section, whereas binding to the plaques in the control section was minimal (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20rodentia%5BMeSH%5D)]

Ono et al. (10) showed that, in normal rat brains, [^11^C]SB-13 had moderate lipophilicity (log(P) = 2.36) and very good brain penetration as well as washout after intravenous injection of the radiotracer.

Initial brain uptake was relatively high in the cortex region (~1.5% of injected dose (ID)/g tissue at 2 min post injection), whereas retention was low in the cerebellum regional brain (~0.3% ID/g tissue at 60 min post injection).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20%28baboon%20OR%20%28primate%20NOT%20human%29%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-N-methylamino-4%27-hydroxystilbene%20AND%20%28human%20NOT%20baboon%29)]

The first human data on [^11^C]SB-13 were obtained by Verhoeff et al. (13), who studied five female AD patients (53-74 years of age) and six healthy females for comparison (54-77 years of age). A 2-h scan was performed after injection of 370 MBq (10 mCi) of either [^11^C]SB-13 or the previously known tracer [^11^C]PIB for comparison. Kinetic analyses were made based on the time–activity curves to obtain Aβ binding-potential estimates, using as input function the unmetabolized tracer concentration in venous plasma (or the density of radioactivity in the cerebellum) from a two-compartment model. As shown previously for [^11^C]PIB, the standardized uptake value (SUV) for [^11^C]SB-13 in the cerebellum (~1.75) appeared similar for both control and AD patients, supporting the fact that the cerebellum could be used as a reference region for nonspecific binding.

For a period of 40-120 min after injection of [^11^C]SB-13 in AD patients, the highest SUVs were obtained in the right striatum (~2.32) and left frontal (~2.35), followed by the right frontal (~2.25) and right thalamus (~2.23). Similar to what was observed for [^11^C]PIB (9, 14), [^11^C]SB-13 displayed good blood–brain barrier permeability and substantial retention in affected cortices (e.g., frontal cortex) of AD patients in comparison with control subjects. The relative cortical uptake was higher for [^11^C]SB-13 than for [^11^C]PIB.

Relatively high specific/nondisplaceable tissue ratios at equilibrium (Rv), with the cerebellum used as reference, were obtained in the association cortices for both tracers. Those results were found consistent with the fact that, in AD patients, the association cortices contain increasingly dense Aβ plaque accumulations. Obtained Rv values for the right striatum were as follows: ~0.32 for [^11^C]SB-13 and ~0.72 for [^11^C]PIB. For the right thalamus, those values were ~0.32 for [^11^C]SB-13 and ~0.51 for [^11^C]PIB.

Verhoeff et al. (13) pointed out several limitations in their study, with respect to the modeling of Aβ binding. The first was the polymerization, diffusion, and degradation of the Aβ plaques. Indeed, although [^11^C]SB-13 likely binds to fibrillar Aβ, there is still controversy about which Aβ species are most important for AD pathogenesis. In addition, the ability of the tracer to penetrate very dense Aβ plaque aggregates likely depends on the shape and size of the plaque.

## References

1 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci, 11 Spec No: p. 213-328.
2 Forstl H, Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R, Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai BJ, Hickey GA, Skoch J, Kajdasz ST, Wang Y, Huang GF, Mathis CA, Klunk WE, Hyman BT. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C, Pike VW, Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K, Small GW, Agdeppa ED, Kepe V, Ercoli LM, Siddarth P, Read S, Satyamurthy N, Petric A, Huang SC, Barrio JR. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk WE, Engler H, Nordberg A, Wang Y, Blomqvist G, Holt DP, Bergstrom M, Savitcheva I, Huang GF, Estrada S, Ausen B, Debnath ML, Barletta J, Price JC, Sandell J, Lopresti BJ, Wall A, Koivisto P, Antoni G, Mathis CA, Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Ono M, Wilson A, Nobrega J, Westaway D, Verhoeff P, Zhuang ZP, Kung MP, Kung HF. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Wilson AA, Garcia A, Jin L, Houle S. (2000). Radiotracer synthesis from [(11)C]-iodomethane: a remarkably simple captive solvent method. Nucl Med Biol.
12 Wilson AA, Jin L, Garcia A, DaSilva JN, Houle S. (2001). An admonition when measuring the lipophilicity of radiotracers using counting techniques. Appl Radiat Isot.
13 Verhoeff NP, Wilson AA, Takeshita S, Trop L, Hussey D, Singh K, Kung HF, Kung MP, Houle S. (2004). In-vivo imaging of Alzheimer disease beta-amyloid with [11C]SB-13 PET. Am J Geriatr Psychiatry.
14 Klunk WE, Engler H, Nordberg A, Bacskai BJ, Wang Y, Price JC, Bergstrom M, Hyman BT, Langstrom B, Mathis CA. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.